# Gallium-68-dotamaleimide-Cys2-annexin A5

Chemical name: | Gallium-68-dotamaleimide-Cys2-annexin A5
Abbreviated name: | ^68^Ga-Cys2-AnxA5
Synonym:
Agent Category: | Proteins
Target: | Phosphatidylserine
Target Category: | Lipids
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | Gallium-68 (^68^Ga)
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=tumor%20responses%20and%20molecular%20imaging)]

The gallium-68 (^68^Ga)-dotamaleimide-Cys2-annexin A5 (AnxA5) conjugate, abbreviated as ^68^Ga-Cys2-AnxA5, is a radionuclide agent developed by Bauwens et al. for phosphatidylserine (PS)-targeted positron emission tomography (PET) of tumor cell apoptosis after chemotherapy and radiotherapy (1). ^68^Ga has a half-life of 68 min and emits positrons with E_max_ β^+^ = 1.9 MeV.

Evaluation of tumor response to therapy is traditionally based on volumetric and morphological changes before and after treatment (2); these changes, however, occur rather late after effective therapy (2). Recent studies have shown that successful treatment induces apoptosis of tumor cells at the very early stage, and externalization of PS is one of the earliest events in apoptosis (3, 4). PS is a membrane phospholipid normally restricted to the inner leaflet of the lipid bilayer. Within a few hours of the apoptotic stimulus, however, PS externalizes to the outer leaflet of the cell membrane and is readily accessible to exogenous molecules. These findings indicate that the early response of tumors to therapy can be evaluated by detection of apoptosis via imaging of externalized PS (2, 3, 5).

AnxA5 is a cellular protein of 36 kDa and specifically binds to membrane-bound PS with nanomolar affinity in the presence of calcium (Ca^2+^) (3, 6, 7). AnxA5 has no immunogenicity or toxicity when used in vivo. These features of AnxA5 make it a valuable agent for in vivo apoptosis detection. AnxA5 was first radiolabeled with ^125^I and later with other radionuclides, including ^99m^Tc, ^18^F, ^111^In, and ^68^Ga (1, 5, 6). Both preclinical and clinical studies have shown that AnxA5-based radionuclides are promising tracers for the rapid dection of apoptosis. However, there are several issues that remain to be resolved (1, 2). First is the suboptimal pharmacokinetics of radiolabeled AnxA5 agents. A high nonspecific accumulation is often observed in the liver and kidneys. Second is the decreased binding affinity caused by radiolabeling and other conjugations. Optimal binding of AnxA5 to PS also requires a micromolar concentration of Ca^2+^. Third is the inability of AnxA5 agents to differentiate apoptosis from necrosis because PS is also externalized during necrosis.

To maintain the binding affinity of AnxA5, Tait et al. applied a site-specific labeling technique in the radiolabeling of AnxA5, and they have shown that specific labeling in the non-binding region of AnxA5 improves the detection of apoptosis compared to random labeling of amino residues (8). Using a similar method, Bauwens et al. synthesized two radionuclide agents, ^68^Ga-Cys2-AnxA5 and ^68^Ga-Cys165-AnxA5 (1). Cys2-AnxA5 and Cys165-AnxA5 are two variants of AnxA5, and they contain a single available Cys residue at the 2-position and at the 165-position, respectively. Both Cys residues are located at the concave side of AnxA5, opposite the convex side that harbors the Ca^2+^/PS binding sites. Covalent coupling of large structures such as liposomes and iron nanoparticles via thiol-chemistry to the Cys2-AnxA5 or Cys165-AnxA5 exhibits no side effect on the PS binding activity (8-11). Bauwens et al. showed that both ^68^Ga-Cys2-AnxA5 and ^68^Ga-Cys165-AnxA5 exhibit a clear binding to apoptotic cells and are promising tracers for the rapid evaluation of cancer therapy (1). No significant differences between the two analogs were observed in the data obtained from in vitro and in vivo analyses. This chapter summarizes the data obtained with ^68^Ga-Cys2-AnxA5, and another chapter in MICAD summarizes the data obtained with ^68^Ga-Cys165-AnxA5.

### Related Resource Links:

- Annexin-based chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=annexin%20AND%20micad%5bbook%5d)
- Protein information of annexins (http://www.ncbi.nlm.nih.gov/protein?term=Annexin)
- Structures of annexins (http://www.ncbi.nlm.nih.gov/structure?term=Annexin)
- Annexin-related compounds in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance?term=Annexin)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=21492787)]

Bauwens et al. described the synthesis of ^68^Ga-Cys2-AnxA5 in detail (1). ^68^Ga was obtained from a titanium dioxide–based ^68^Ge/^68^Ga generator, and ^68^Ga-dotamaleimide was synthesized by heating a mixture of ^68^Ga and dotamaleimide for 8 min at 90°C. Cys2-AnxA5 was produced by site-directed mutagenesis of human AnxA5 cDNA and expressed in Escherichia coli (purity >95%). The introduction of Cys2 did not affect the Ca^2+^-dependent PS binding. To couple with ^68^Ga-dotamaleimide, Cys2-AnxA5 was treated with dithiothreitol to convert all potentially formed disulfide bridges to free thiols. The ^68^Ga-dotamaleimide and AnxA5 variant were then mixed, incubated for 15 min at 37°C, and purified. This step resulted in a coupling yield (radiochemical yield) of 70 ± 10%. Purification led to a loss of ~10%; the radiochemical purity was >98%. The total synthesis time was ~55 min, with an end-of-synthesis yield of 25% (43% decay-corrected). ^68^Ga-Cys2-AnxA5 was stable for at least 1.5 h in vitro in HEPES buffer and in plasma, both at 25°C and at 37°C. No free ^68^Ga, ^68^Ga-dotamaleimide, or any other metabolites could be detected.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=21492787)]

The in vitro binding capacity of ^68^Ga-Cys2-AnxA5 was evaluated with Jurkat cells after anti-Fas treatment (1). Jurkat cells have been shown to expose PS upon treatment with anti-Fas (12). The total activity bound to anti-Fas–treated Jurkat cells (66.6 ± 2.1%) was approximately five times higher than the total activity bound to untreated cells (11.7 ± 0.4%), indicating a well-preserved PS binding capacity. No blocking studies were reported.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=21492787)]

Dynamic PET imaging was first performed in healthy Naval Medical Research Institute (NMRI) mice (n = 4) after tail vein injection of ^68^Ga-Cys2-AnxA5 (7–15 MBq (0.19–0.41 mCi)) (1). Images revealed a fast clearance of the tracer from the blood toward the kidneys, with no significant change in biodistribution from 30 min to 60 min after injection. The blood half-life of ^68^Ga-Cys2-AnxA5 was 6.5 min. Dissection data of the organs confirmed that ^68^Ga-Cys2-AnxA5 was cleared mainly via the urinary tract. A high percentage of activity was retained in the kidneys, in particular in the cortex, with only limited clearance toward the urinary bladder. Analysis of plasma and urine samples indicated that no radioactive metabolites could be detected in the plasma of the animal, whereas activity in the urine was only in the form of radiolabeled metabolites, likely small ^68^Ga-dotamaleimide-Cys adducts. Minor uptake was also observed in the liver, intestines, spleen, and lungs. Detection of apoptosis with ^68^Ga-Cys2-AnxA5 was performed in anti-Fas–treated animals (n = 4) (1). Anti-Fas monoclonal antibody (mAb) treatment induces apoptosis in normal organs, especially the liver. NMRI mice were pretreated with 0.2 μg/g purified hamster anti-Fas mAb for 90 min, at which time the mice were injected via the tail vein with 7–15 MBq (0.19–0.41 mCi) ^68^Ga-Cys2-AnxA5. Images were obtained at 1 h after injection, and the accumulation in organs was calculated and expressed as a percentage of injected dose per organ (% ID/organ). The ^68^Ga-Cys2-AnxA5 showed a major shift of the radioactivity from the kidneys to the apoptotic liver. There was a significant difference in the amount of ^68^Ga-Cys2-AnxA5 in the organs of healthy mice compared with that in the organs of anti-Fas–treated mice: liver, 6.86 ± 0.41 (normal) versus 51.0 ± 3.1 (treated); kidneys, 75.9 ± 1.6 (normal) versus 26.4 ± 5.3 (treated); lungs, 0.33 ± 0.04 (normal) versus 0.76 ± 0.17 (treated); and spleen, 0.87 ± 0.08 (normal) versus 1.65 ± 0.32 (treated). The higher uptake in apoptotic liver tissue was further confirmed with autoradiography of the liver slices dissected 1 h after injection.

The feasibility of ^68^Ga-Cys2-AnxA5 in the detection of apoptosis after chemotherapy and radiotherapy was tested in animals bearing lymphoma xenografts (Daudi, a human B-lymphoblast cell line) (1). Animals were treated with cyclophosphamide (125 mg/kg) 1 day before imaging and then with radiation (10 Gy/tumor) 4–6 h before imaging. Dynamic PET imaging was performed 1 h after injection of 7–15 MBq (0.19–0.41 mCi) ^68^Ga-Cys2-Anx (n = 3). This was done before and after treatment of the animals. PET images showed no clear difference in the biodistribution of ^68^Ga-Cys2-AnxA5 between the healthy and tumor-bearing animals. The uptake in the tumor was minimal, but MRI-PET fusion images demonstrated clear delineation of each tumor. The standardized uptake values (SUV_mean_) were then calculated with the following formula: SUV = measured activity concentration in the tumor (Bq/g) × body weight (g) ÷ injected activity (Bq). The after-therapy SUV values significantly exceeded (P < 0.05) those prior to therapy: 0.141 ± 0.039 versus 0.092 ± 0.028 for SUV_10min_; 0.084 ± 0.005 versus 0.047 ± 0.005 for SUV_30min_; and 0.076 ± 0.003 versus 0.041 ± 0.008 for SUV_60min_. These findings were confirmed with the dissection data at 1 h after injection, which showed that the tumor uptake was significantly higher in the treated animals than in the untreated animals (0.141 ± 0.022% ID/g tissue versus 0.046 ± 0.002% ID/g tissue). Autoradiography of the tumor slices also showed increased activity in the treated tumors. The apoptosis in the tumor tissue seemed very inhomogeneous as several regions showed an uptake 10–20 times higher than the tumor uptake prior to treatment, whereas other regions were relatively unaffected (1). Blocking studies in the treated animals were not reported.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Bauwens M., De Saint-Hubert M., Devos E., Deckers N., Reutelingsperger C., Mortelmans L., Himmelreich U., Mottaghy F.M., Verbruggen A. (2011). Site-specific 68Ga-labeled Annexin A5 as a PET imaging agent for apoptosis. Nucl Med Biol.
2 Neves A.A., Brindle K.M. (2006). Assessing responses to cancer therapy using molecular imaging. Biochim Biophys Acta.
3 Schutters K., Reutelingsperger C. (2010). Phosphatidylserine targeting for diagnosis and treatment of human diseases. Apoptosis.
4 Nguyen Q.D., Aboagye E.O. (2010). Imaging the life and death of tumors in living subjects: Preclinical PET imaging of proliferation and apoptosis. Integr Biol (Camb).
5 Kapty J., Murray D., Mercer J. (2010). Radiotracers for noninvasive molecular imaging of tumor cell death. Cancer Biother Radiopharm.
6 Kuge Y., Zhao S., Takei T., Tamaki N. (2009). Molecular imaging of apoptosis with radio-labeled Annexin A5 focused on the evaluation of tumor response to chemotherapy. Anticancer Agents Med Chem.
7 Niu G., Chen X. (2010). Apoptosis imaging: beyond annexin V. J Nucl Med.
8 Tait J.F., Smith C., Levashova Z., Patel B., Blankenberg F.G., Vanderheyden J.L. (2006). Improved detection of cell death in vivo with annexin V radiolabeled by site-specific methods. J Nucl Med.
9 De Saint-Hubert M., Mottaghy F.M., Vunckx K., Nuyts J., Fonge H., Prinsen K., Stroobants S., Mortelmans L., Deckers N., Hofstra L., Reutelingsperger C.P., Verbruggen A., Rattat D. (2010). Site-specific labeling of 'second generation' annexin V with 99mTc(CO)3 for improved imaging of apoptosis in vivo. Bioorg Med Chem.
10 van Tilborg G.A., Mulder W.J., Deckers N., Storm G., Reutelingsperger C.P., Strijkers G.J., Nicolay K. (2006). Annexin A5-functionalized bimodal lipid-based contrast agents for the detection of apoptosis. Bioconjug Chem.
11 Li X., Link J.M., Stekhova S., Yagle K.J., Smith C., Krohn K.A., Tait J.F. (2008). Site-specific labeling of annexin V with F-18 for apoptosis imaging. Bioconjug Chem.
12 Green A.M., Steinmetz N.D. (2002). Monitoring apoptosis in real time. Cancer J.